# ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Ac-RWQPCPAESWT-Cha-CWDPGGGK-NH_2_ (FibPep)

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Ac-RWQPCPAESWT-Cha-CWDPGGGK-NH_2_ (FibPep)
Abbreviated name: | ^111^In-DOTA-FibPep
Synonym:
Agent category: | Peptide
Target: | Fibrin
Target category: | Acceptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FibPep)]

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). A meshwork of clotted plasma protein is present in the tumor stroma but not in normal tissues, providing a functional matrix for angiogenesis, cell migration, and tumor cell invasion (3). There are high levels of collagens, fibronectin, and fibrin in the tumor connective tissues.

Thrombosis plays a major role in many cardiovascular diseases such as myocardial infarction, pulmonary embolism, deep venous thrombosis, and cerebral venous thrombosis (4). Thrombosis occurs by an activation process of thrombin (F2 coagulation factor II), which then converts fibrinogen into fibrin. Thrombin initiates the cross-linking of the polymerized fibrin via the activation of a transglutamase enzyme called coagulation factor XIII (FXIIIa indicates activated factor XIII) (5). Atherosclerotic lesions often contain microthrombi and fibrin on their surface (6). Fibrin is associated with a variety of malignant tumors (7). Fibrin is essential for stroma formation in the tumor with deposition of fibrin, which leads to tumor angiogenesis and metastasis. The cyclic fibrin-binding peptide Ac-RWQPCPAESWT-Cha-CWDPGGGK-NH_2_ (FibPep), containing the fibrin-binding motif RWQPCPAESWT-Cha-CWDP (previously identified via phage-display screening) was radiolabeled with ^111^In via 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA) conjugation to the N-terminal Lys (^111^In-DOTA-FibPep) for use with single-photon emission computed tomography (SPECT) imaging of fibrin (8).

### Related Resource Links:

- Chapters in MICAD (fibrin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Fibrin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (fibrinogen (http://www.ncbi.nlm.nih.gov/gene/2243), thrombin (http://www.ncbi.nlm.nih.gov/gene/2147))
- Articles in Online Mendelian Inheritance in Man (OMIM) (fibrinogen (http://www.ncbi.nlm.nih.gov/omim/134820), thrombin (http://omim.org/entry/176930))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FibPep+synthesis)]

FibPep and a scrambled negative control Ac-WPTAD-Cha-RAWPSQEWPAGGGK-NH_2_ (NCFibPep) were prepared with solid-phase peptide synthesis (8). These peptides were incubated with a 7-fold excess of DOTA-NHS ester for 18 h at room temperature. DOTA-FibPep and DOTA-NCFibPep were purified with high-performance liquid chromatography, and their expected molecular weights were confirmed with mass spectrometry. There was on average one DOTA moiety per conjugate. Radiolabeling with ^111^InCl_3_ in ammonium acetate buffer (pH 6) for 60 min at 75°C resulted in >95% yield and radiochemical purity for both peptides. Specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FibPep+in+vitro)]

In vitro binding studies showed that ^111^In-DOTA-FibPep exhibited significantly higher binding than ^111^In-DOTA-NCFibPep and free ^111^In to fibrin (85.8, 1.2, and 2.1% dose, respectively) and to blood clots (32.2, 5.1, and 1.0% dose, respectively) (n = 4, P < 0.01) (8). ^111^In-DOTA-FibPep bound with affinity to fibrin, with a dissociation constant (K_d_) of 0.8 ± 0.1 µM and 2.8 ± 0.1 binding sites per fibrin molecule (n = 4). ^111^In-DOTA-NCFibPep exhibited ~100-fold weaker binding to fibrin than ^111^In-DOTA-FibPep.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FibPep+rodentia)]

Starmans et al. (8) performed ex vivo biodistribution studies in normal mice (n = 4/group) after injection of 1.13 MBq (0.031 mCi, 15 nmol) ^111^In-DOTA-FibPep or ^111^In-DOTA-NCFibPep. Both peptides showed biphasic blood distribution. ^111^In-DOTA-FibPep exhibited a distribution half-life (t_1/2α_) of 1 min and an elimination t_1/2β_ of 16 min, resulting in <1% injected dose per gram (ID/g) at 90 min. ^111^In-DOTA-NCFibPep exhibited the distribution t_1/2α_ of 2 min and elimination t_1/2β_ of 20 min, resulting in <2% injected dose per gram (ID/g) at 90 min. The biodistribution profile at 4 h after injection showed low accumulation of radioactivity in the major organs (<1.4% ID/g), with the highest radioactivity in the kidneys (7.1 ± 0.9% ID/g for ^111^In-DOTA-FibPep and 12.9 ± 4.2% ID/g for ^111^In-DOTA-NCFibPep). No blocking studies were performed.

SPECT imaging studies were performed at 90, 115, 137, and 162 min after injection of 37 MBq (1 mCi, 15 nmol) ^111^In-DOTA-FibPep or ^111^In-DOTA-NCFibPep in mice (n = 4/group) with the right carotid artery exposed and treated with 10% FeCl_3_ solution to induce thrombosis (8). ^111^In-DOTA-FibPep exhibited high signal intensity (22.5 counts/voxel) in the thrombus-containing carotid artery at 90 min, and the intensity gradually declined to 15 counts/voxel at 162 min. On the other hand, ^111^In-DOTA-NCFibPep exhibited lower signal intensities of ~5 counts/voxel at 90, 115, 137, and 162 min (P < 0.02). The muscle showed low signal intensities (<2.5 counts/voxel) with both tracers at these time points. Both tracers showed radioactivity only in the kidneys and urinary bladder, suggesting renal elimination. Ex vivo analysis of the carotid arteries at 3.5 h after injection exhibited significantly higher (P < 0.01) accumulation of ^111^In-DOTA-FibPep in the injured carotid than in the non-injured carotid and in muscle (5.7 ± 0.7%, 0.6 ± 0.4%, and 0.2 ± 0.2% ID/g, respectively). Accumulation of ^111^In-DOTA-NCFibPep in the injured carotid was similar to that in the non-injured carotid and in muscle (0.4 ± 0.2%, 0.3 ± 0.01%, and 0.1 ± 0.1% ID/g, respectively). Histological staining confirmed the presence of thrombus in the injured carotid. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FibPep+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FibPep+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FibPep+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
4 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
5 Lee K.N., Lee C.S., Tae W.C., Jackson K.W., Christiansen V.J., McKee P.A. (2001). Crosslinking of alpha 2-antiplasmin to fibrin. Ann N Y Acad Sci.
6 Constantinides P. (1990). Cause of thrombosis in human atherosclerotic arteries. Am J Cardiol.
7 Rickles F.R., Patierno S., Fernandez P.M. (2003). Tissue factor, thrombin, and cancer. Chest.
8 Starmans L.W., van Duijnhoven S.M., Rossin R., Aime S., Daemen M.J., Nicolay K., Grull H. (2013). SPECT imaging of fibrin using fibrin-binding peptides. Contrast Media Mol Imaging.